# ^68^Ga-1,4,7-Triazacyclononane-1,4-7-triacetic acid-Glu-[Gly-Gly-Gly-c(Arg-Gly-Asp-D-Phe-Lys)]_2_

Chemical name: | ^68^Ga-1,4,7-Triazacyclononane-1,4-7-triacetic acid-Glu-[Gly-Gly-Gly-c(Arg-Gly-Asp-D-Phe-Lys)]_2_
Abbreviated name: | ^68^Ga-NOTA-G_3_-RGD2, ^68^Ga-NOTA-E-[G-G-G-c(RGDfK)]_2_
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. The α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). The peptide sequence Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most of the cyclic RGD peptides are composed of five amino acids. Various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (50% inhibition concentration (IC_50_), 7–40 nM) but not to α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM) integrins (11). Various radiolabeled cyclic RGD peptides and peptidominetics have been found to have high accumulation in tumors in mice (12, 13). Out of these developments [^18^F]Galacto-c(RGDfK) has been evaluated in a number of clinical studies for imaging of α_v_β_3_ in cancer patients (14-19). Li et al. (20) used 1,4,7-triazacyclononane-1,4-7-triacetic acid (NOTA) as a bifunctional chelator for labeling Glu-[Gly-Gly-Gly-cyclo(RGDfK)]_2_ (G_3_-RGD2) to form (^68^Ga-NOTA-G_3_-RGD2) for positron emission tomography (PET) imaging of α_v_β_3_ receptors in nude mice bearing human glioblastoma U87MG tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+synthesis)]

G_3_-RGD2 was prepared with solid-phase peptide synthesis (20). Addition of the NOTA group to G_3_-RGD2 was performed by mixing 2 µmol RGD2 with 6 μmol S-2-(4-isothiocyanatobenzyl)-NOTA in sodium bicarbonate buffer (pH 9) for 5 h at room temperature. NOTA-G_3_-RGD2 was isolated with high-performance liquid chromatography (HPLC) with 43% yield and >95% purity. Molecular weight was determined with MALDI-TOF-MS to be m/z 2,112.97 Da (calculated molecular weight, 2,110.95 Da). For ^68^Ga labeling, a solution of 185 MBq (5 mCi) ^68^GaCl_3_ and 10 nmol RGD2 was heated for 10 min at 42°C. ^68^Ga-NOTA-RGD2 was purified with HPLC with a yield of 92% and a radiochemical purity of >98%. The specific activity was 9.8–11.8 MBq/nmol (0.26–0.32 mCi/nmol) at the end of purification.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+in+vitro)]

Liu et al. (20) performed in vitro inhibition studies of NOTA-RGD2 in cultured human U87MG cells with ^125^I-echistatin. The IC_50_ values were 88.8, 61.6, 100.0, and 66.4 nM for RGD2, G_3_-RGD2, NOTA-RGD2, and NOTA-G_3_-RGD2, respectively. These comparable IC_50_ values indicated that NOTA and G_3_ conjugation had little effect on the receptor binding affinity.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+%20rodentia)]

Liu et al. (20) performed ex vivo biodistribution studies of 0.37 MBq (10 μCi) ^68^Ga-NOTA-G_3_-RGD2 or ^68^Ga-NOTA-RGD2 in nude mice bearing U87MG xenografts at 1 h after injection. Tumor accumulation was 7.05 ± 1.06% and 4.17 ± 1.10% injected dose per gram (ID/g) for ^68^Ga-NOTA-G_3_-RGD2 and ^68^Ga-NOTA-RGD2, respectively. The tumor/muscle ratios were 8.5 and 2.9 for ^68^Ga-NOTA-G_3_-RGD2 and ^68^Ga-NOTA-RGD2, respectively. Therefore, the G_3_-linkers improved the tumor pharmacokinetics. The kidney accumulation was 10.9% ID/g for ^68^Ga-NOTA-G_3_-RGD2 and 11.1% ID/g for ^68^Ga-NOTA-RGD2. Quantitative analyses of PET imaging data showed that the radioactivity levels in the U87MG tumors (n = 4 mice) were 9.04 ± 2.05% ID/g (30 min), 7.36 ± 2.08% ID/g (60 min), and 6.38 ± 1.31% ID/g (120 min) for ^68^Ga-NOTA-G_3_-RGD2. ^68^Ga-NOTA-RGD2 was excreted mainly through the kidneys. Coinjection of c(RGDyK) and ^68^Ga-NOTA-G3-RGD2 reduced the tumor accumulation to the background level with ~80% inhibition at 60 min after injection. The tumor/muscle, tumor/liver, tumor/blood, and tumor/kidney ratios for ^68^Ga-NOTA-G3-RGD2 were significantly higher than those for ^68^Ga-NOTA-RGD2 (P < 0.01) at the three time points.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Haubner R., Decristoforo C. (2009). Radiolabelled RGD peptides and peptidomimetics for tumour targeting. Front Biosci.
13 Schottelius M., Laufer B., Kessler H., Wester H.J. (2009). Ligands for mapping alphavbeta3-integrin expression in vivo. Acc Chem Res.
14 Beer A.J., Grosu A.L., Carlsen J., Kolk A., Sarbia M., Stangier I., Watzlowik P., Wester H.J., Haubner R., Schwaiger M. (2007). [18F]galacto-RGD positron emission tomography for imaging of alphavbeta3 expression on the neovasculature in patients with squamous cell carcinoma of the head and neck. Clin Cancer Res.
15 Beer A.J., Haubner R., Goebel M., Luderschmidt S., Spilker M.E., Wester H.J., Weber W.A., Schwaiger M. (2005). Biodistribution and pharmacokinetics of the alphavbeta3-selective tracer 18F-galacto-RGD in cancer patients. J Nucl Med.
16 Beer A.J., Haubner R., Sarbia M., Goebel M., Luderschmidt S., Grosu A.L., Schnell O., Niemeyer M., Kessler H., Wester H.J., Weber W.A., Schwaiger M. (2006). Positron emission tomography using [18F]Galacto-RGD identifies the level of integrin alpha(v)beta3 expression in man. Clin Cancer Res.
17 Beer A.J., Lorenzen S., Metz S., Herrmann K., Watzlowik P., Wester H.J., Peschel C., Lordick F., Schwaiger M. (2008). Comparison of integrin alphaVbeta3 expression and glucose metabolism in primary and metastatic lesions in cancer patients: a PET study using 18F-galacto-RGD and 18F-FDG. J Nucl Med.
18 Beer A.J., Niemeyer M., Carlsen J., Sarbia M., Nahrig J., Watzlowik P., Wester H.J., Harbeck N., Schwaiger M. (2008). Patterns of alphavbeta3 expression in primary and metastatic human breast cancer as shown by 18F-Galacto-RGD PET. J Nucl Med.
19 Haubner R., Weber W.A., Beer A.J., Vabuliene E., Reim D., Sarbia M., Becker K.F., Goebel M., Hein R., Wester H.J., Kessler H., Schwaiger M. (2005). Noninvasive visualization of the activated alphavbeta3 integrin in cancer patients by positron emission tomography and [18F]Galacto-RGD. PLoS Med.
20 Liu Z., Niu G., Shi J., Liu S., Wang F., Liu S., Chen X. (2009). (68)Ga-labeled cyclic RGD dimers with Gly3 and PEG4 linkers: promising agents for tumor integrin alphavbeta3 PET imaging. Eur J Nucl Med Mol Imaging.